# MFE23-Cy5 anti-carcinoembryonic antigen trimerbody

Chemical name: | MFE23-Cy5 anti-carcinoembryonic antigen trimerbody
Abbreviated name: | MFE23-Cy5 anti-CEA trimerbody
Synonym:
Agent Category: | Antibody
Target: | Carcinoembryonic antigen (CEA)
Target Category: | Antigen
Method of detection: | Near-infrared fluorescence (NIR) imaging
Source of signal / contrast: | Cy5
Activation: | No
Studies: | - In vitro; - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CEA%20AND%20tumor%20AND%20imaging%20AND%20antibody)]

Carcinoembryonic antigen (CEA) is a marker of tumor prognosis, staging, recurrence, metastasis, and treatment response. MFE23-Cy5 anti-CEA trimerbody is an anti-CEA single-chain variable fragment (scFv) trimerbody labeled with the fluorescent reporter Cy5, and it has been developed for optical imaging of CEA-positive tumors (1).

Monoclonal antibodies (mAbs) and antibody fragments have been used for tumor targeting for many years. An ideal tumor-targeting antibody should fulfill several requirements: rapid tissue penetration, high target retention, and rapid blood clearance (2, 3). The format and molecular weight of an antibody are critical factors that influence its pharmacokinetics and in vivo efficacy (2-4). Intact mAbs (~150 kDa) display low blood clearance and incomplete tumor penetration. The production yield of mAbs is limited (2). These disadvantages of mAbs are partially overcome by developing recombinant scFv antibody fragments. Monovalent scFv (25–30 kDa) represents the smallest functional component of an antibody, and it is more efficient in tumor penetration. However, the scFv fragment is cleared from blood too rapidly, and it has poor binding affinity and tumor retention. Bivalent antibodies such as diabodies (55–60 kDa) and minibodies (~80 kDa) possess more ideal tumor-targeting characteristics such as compact size and higher binding affinity than monovalent scFv (3). Diabodies are dimeric molecules consisting of two scFv fragments connected with a short linker. Minibodies are formed by the fusion of scFv fragments with the IgG1 CH3 domain. Improved affinity of the bivalent antibodies relies on binding and rebinding, as well as simultaneous binding to different molecules of the antigen (1, 5). An issue is that it will lead to small gains in functional affinity if simultaneous multiple binding is not sterically possible. Taking the advantages of collagen XVIII NC1 domain and scFv fragments, Sanchez-Arévalo Lobo et al. developed a multivalent antibody, termed “trimerbody,” for in vivo tumor targeting (5). The NC1 domain of collagen XVIII consists of three functionally different subdomains: an N-terminal noncovalent trimerization subdomain implicated in self-assembly of homotrimers, a central protease-sensitive hinge region, and a compact C-terminal endostatin globular subdomain (1, 5, 6). The trimerbody is designed and constructed by connecting scFv fragments to the N-terminal trimerization subdomains of NC1 through flexible linkers. The resulting trimerbody has a tripod-shaped structure with three scFv heads oriented radially outward. The artificial linker between the N-terminal scFv and NC1 domain consisted of 21 amino acids. The maximal length of the linker is 79.8 Å if the conformation is fully extended, which allows the scFv heads to be highly flexible and provides numerous binding geometries (1, 5). Based on the concept of the trimerbody construction, Cuesta et al. constructed a fluorescently labeled MFE23-Cy5 anti-CEA trimerbody (1). CEA is a 180-kDa glycoprotein, and it is involved in cell adhesion and is localized in the apical surface of mature enterocytes (7). In a majority of cancers from the colorectum, stomach, pancreas, breast, and lung, as well as several other carcinomas of epithelial origin, CEA is overexpressed and has been used as a marker of tumor prognosis, staging, recurrence, metastasis, and treatment response (8-12). With optical imaging, Cuesta et al. demonstrated that the MFE23-Cy5 anti-CEA trimerbody was well localized the tumors after systemic administration to the mice bearing CEA-positive tumor xenografts (1).

Based on the same design concept, the trimerbody targeting the laminin epitope (L36-Cy5 anti-laminin trimerbody (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)) was also constructed and analyzed for its feasibility in imaging fibrosarcomas and adenocarcinomas (1, 5).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=laminin%20AND%20trimerbody)]

The synthesis of the MFE23-Cy5 anti-CEA trimerbody and B1.8-Cy5 anti-hapten 4-hydroxy-5-iodo-3-nitrophenyl (anti-NIP) trimerbody (used as control) was described in detail by Cuesta et al. and Sanchez-Arévalo Lobo et al., separately (1, 5). The plasmids of pCEP4-B1.8, pCR3.1-L36-NC1^ES-^, and pVOM1.C23 were used to construct the trimerbody expression vectors. Plasmid pCEP4-B1.8 contains the B1.8 anti-NIP scFv gene and the polyhistidine and c-Myc epitopes. pCR3.1-L36-NC1^ES-^ contains the L36 anti-laminin scFv gene and the NC1 trimerization subdomain. The plasmid pVOM1.C23 contains the MFE23 anti-human CEA scFv gene. The MFE23 expression cassette from the plasmid pVOM1.C23 was subcloned into the vector pCEP4.6xHis-Myc, resulting in the plasmid of pCEP4-MFE23. The NC1 trimerization domain (a 252-bp fragment) was first amplified from the plasmid pCR3.1-L36-NC1^ES-^ and then ligated into the plasmids pCEP4-MFE23 and pCEP4-B1.8, resulting in the expression plasmids pCEP4-MFE23-NC1^ES-^ and pCEP4-B1.8-NC1^ES-^, respectively. To express the trimerbodies, HEK-293 (human embryo kidney epithelia) cells were transfected with the expression plasmids pCEP4-MFE23-NC1^ES-^ and pCEP4-B1.8-NC1^ES-^, separately. Stably transfected HEK-293 cell lines were established through hygromycin B selection. The trimerbodies were isolated in a functionally active form from the serum-free conditioned medium of the transfected HEK293 cells, and they were purified with immobilized metal affinity chromatography. Purified trimerbodies were labeled with Cy5 N-hydroxysuccinimde esters. The labeling ratio of Cy5/trimerbody was close to 1:1. The purity of the yielded trimerbodies was >95%. The trimeric nature of the trimerbodies was confirmed with ultracentrifugation and analytical gel filtration chromatography. The molecular weights of MFE23-Cy5 anti-CEA trimerbody and B1.8-Cy5 anti-NIP trimerbody were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=laminin%20AND%20trimerbody)]

The functionality of the trimerbodies was investigated against plastic immobilized NIP-BSA conjugates (NIP_10_-BSA), human CEA, and the CEA antigen in a cellular context with ELISA and flow cytometry (1, 5). The results demonstrated that the trimerbodies recognized not only immobilized antigen but also native antigen on the surface of tumor cells. Positive staining with MFE-23 trimerbody was observed for the CEA-positive HeLa^CEA^ (human cervix carcinoma) cells but not for CEA-negative HeLa cells. Staining with B1.8 trimerbody revealed no specific signal for either CEA-positive or CEA-negative cells. Surface plasmon resonance analysis demonstrated that the anti-NIP trimerbody had a higher binding signal and slower dissociation than the corresponding monomeric antibody, consistent with multivalent binding to the antigen. The anti-NIP trimerbody had at least a 100-fold increase in functional affinity to NIP_10_-BSA antigen compared with its monovalent counterpart. The detailed binding affinity and in vitro stability of the anti-CEA trimerbody were not reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=laminin%20AND%20trimerbody)]

The potential of the MFE23-Cy5 anti-CEA trimerbody for in vivo targeting was assessed in nude mice bearing human tumor xenografts (1). MKN45 (human stomach adenocarcinoma), HT1080 (human fibrosarcoma), or HeLa cells were implanted subcutaneously into the dorsal space of 6-week-old female Hsd:athymic nude-Foxn1^nu^ mice (n = 4/group). Mice were injected with 100 µl Cy5-labeled trimerbody in phosphate-buffered saline (5 mg/kg) through the tail vein. Optical imaging showed that the MFE23-Cy5 anti-CEA trimerbody localized rapidly and specifically to CEA-positive MKN45 tumor xenografts. The tumor uptake reached a maximum at 3 h after injection and slowly washed out over time. The fluorescence was still detectable in the tumors at 48 h after injection. The control B1.8-Cy5 anti-NIP trimerbody showed no detectable localization in any of the three tumor types. The biodistribution of the MFE23-Cy5 anti-CEA trimerbody was not reported. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Cuesta A.M., Sanchez-Martin D., Sanz L., Bonet J., Compte M., Kremer L., Blanco F.J., Oliva B., Alvarez-Vallina L. (2009). In vivo tumor targeting and imaging with engineered trivalent antibody fragments containing collagen-derived sequences. PLoS One.
2 Gronwall C., Stahl S. (2009). Engineered affinity proteins--generation and applications. J Biotechnol.
3 Chames P., Baty D. (2009). Bispecific antibodies for cancer therapy. Curr Opin Drug Discov Devel.
4 Friedman M., Stahl S. (2009). Engineered affinity proteins for tumour-targeting applications. Biotechnol Appl Biochem.
5 Sanchez-Arevalo Lobo V.J., Cuesta A.M., Sanz L., Compte M., Garcia P., Prieto J., Blanco F.J., Alvarez-Vallina L. (2006). Enhanced antiangiogenic therapy with antibody-collagen XVIII NC1 domain fusion proteins engineered to exploit matrix remodeling events. Int J Cancer.
6 Ortega N., Werb Z. (2002). New functional roles for non-collagenous domains of basement membrane collagens. J Cell Sci.
7 Marshall J. (2003). Carcinoembryonic antigen-based vaccines. Semin Oncol.
8 Duffy M.J. (2001). Carcinoembryonic antigen as a marker for colorectal cancer: is it clinically useful?. Clin Chem.
9 Goldstein M.J., Mitchell E.P. (2005). Carcinoembryonic antigen in the staging and follow-up of patients with colorectal cancer. Cancer Invest.
10 Kenanova V., Barat B., Olafsen T., Chatziioannou A., Herschman H.R., Braun J., Wu A.M. (2009). Recombinant carcinoembryonic antigen as a reporter gene for molecular imaging. Eur J Nucl Med Mol Imaging.
11 Kuroki M., Hachimine K., Huang J., Shibaguchi H., Kinugasa T., Maekawa S. (2005). Re-targeting of cytotoxic T lymphocytes and/or natural killer cells to CEA-expressing tumor cells with anti-CEA antibody activity. Anticancer Res.
12 Tan E., Gouvas N., Nicholls R.J., Ziprin P., Xynos E., Tekkis P.P. (2009). Diagnostic precision of carcinoembryonic antigen in the detection of recurrence of colorectal cancer. Surg Oncol.